# Cy7-(3S,7S)-26-Amino-5,13,20-trioxo-4,6,12,21-tetraazahexacosane-1,3,7,22-tetracarboxylic acid

Chemical name: | Cy7-(3S,7S)-26-Amino-5,13,20-trioxo-4,6,12,21-tetraazahexacosane-1,3,7,22-tetracarboxylic acid
Abbreviated name: | Cy7-3
Synonym:
Agent category: | Compound
Target: | Prostate-specific membrane antigen (PSMA), or N-acetyl α-linked acidic dipeptidase (NAALADase)
Target category: | Antigen
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | Cy7
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4758398), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4758397) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2346) for more information about PSMA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy7-3)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-4). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–650 nm) are used. Near-infrared (NIR) fluorescence (650–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a noninvasive alternative to radionuclide imaging in small animals (4, 5).

Prostate-specific membrane antigen (PSMA) is a cell-surface glycoprotein with a molecular weight of ~100 kDa. It is a unique, type II, transmembrane-bound glycoprotein that is overexpressed on prostate tumor cells and in the neovasculature of most solid prostate tumors, but not in the vasculature of normal tissues (6, 7). PSMA has also been detected in other tissues such as the kidneys, the proximal small intestine, and the salivary glands (7). PSMA was found to have N-acetyl α-linked acidic dipeptidase (NAALADase) or glutamate carboxypeptidase II activity (8). PSMA may play an important role in the progression of prostate cancer and glutamatergic neurotransmission, as well as in the absorption of folate (9). In the central nervous system, PSMA metabolizes N-acetyl-aspartyl-glutamate, and in the proximal small intestine it removes γ-linked glutamates from poly-γ-glutamate folate and folate hydrolase (7). PSMA can be used as a marker for the detection of metastatic cancers with imaging agents. Although a commercially available monoclonal antibody (^111^In-labeled Capromomab pendetide (^111^In-CYT-356)) is in clinical use for the detection of prostate cancer, the results obtained with this antibody are not entirely reliable (10). In addition, this IgG antibody has limited access to tumors and also may produce low signal/noise ratios because the target is the intracellular domain of PSMA (11, 12). IRDye800CW-(3S,7S)-26-Amino-5,13,20-trioxo-4,6,12,21-tetraazahexacosane-1,3,7,22-tetracarboxylic acid (YC-27, also known as 800CW-3) is a small molecule inhibitor of NAALADase (13). YC-27 was able to visualize PSMA-positive tumors in nude mice, but accumulation of signal was high in the kidney. Chen et al. (14) evaluated a series of dye-3 conjugates with Cy5.5, IGC, IRDye800RS, and Cy7 in nude mice bearing human PSMA-positive xenografts. Injected Cy7-3 exhibited good tumor accumulation with lower liver and kidney accumulation than YC-27.

### Related Resource Links:

- Chapters in MICAD (PSMA (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PSMA+AND+micad%5Bbook%5D))
- Gene information in NCBI (PSMA (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2346))
- Articles in OMIM Articles in Online Mendelian Inheritance in Man (OMIM) (PSMA (http://omim.org/entry/602640))
- Clinical trials (PSMA (http://www.clinicaltrials.gov/ct2/results?term=PSMA))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy7-3%20AND%20synthesis)]

N,N-Diisopropylethylamine (0.0115 mM) was added to a solution of compound 3 (710 nmol) in dimethyl sulfoxide, followed by N-hydroxysuccininide ester of Cy7 (610 nM) (14). The mixture was incubated at room temperature for 2 h. Cy7-3 was purified with high-performance liquid chromatography with 64% yield. The molecular weight of Cy7-3 (1.27 kDa) with one Cy7 per targeting molecule was confirmed with mass spectroscopy. Cy7-3 exhibited an absorbance maximum at 743 nm and an emission maximum at 767 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy7-3%20AND%20in%20vitro)]

The binding affinity of Cy7-3 for PSMA was determined with the use of a NAALADase assay (14). Cy7-3 exhibited an inhibition constant (K_i_) value of 5.0 ± 0.2 nM. The K_i_ value of 800CW-3 was 20 ± 5 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy7-3%20and%20rodentia)]

Chen et al. (14) performed NIR fluorescence imaging studies of Cy7-3 or YC-27 (1 nmol) in nude mice (n = 3) bearing PSMA-positive PC3-PIP tumor xenografts and PSMA-negative PC3-flu tumor xenografts. The PC3-PIP tumors were clearly visualized at 24 h after injection of the tracers. On the other hand, the NIR signal from the PC3-flu tumors was weak. Kidney accumulation of fluorescence was more prominent for YC-27 than Cy7-3. The tumor/kidney ratio for Cy7-3 was higher than that for YC-27. Ex vivo NIR imaging showed that the PC3-PIP tumors exhibited higher fluorescence intensity than the kidneys, liver, spleen, intestines, and PC3-flu tumors for Cy7-3. Co-injection of 1 nmol Cy7-3 with 1,000 nmol DClBzL (a PSMA inhibitor) in mice bearing the two tumors inhibited the NIR fluorescence in the PC3-PIP tumors nearly to the background level of the PC3-flu tumors at 24 h after injection. The ex vivo NIR signals in the tumors were consistent with the in vivo imaging.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy7-3%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=YC-27%20AND%20Primates)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy7-3%20AND%20human)]

No publication is currently available.

## NIH Support

R01 CA134675

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Leung K., Chopra A., Shan L., Eckelman W.C., Menkens A.E. (2012). Essential parameters to consider for the characterization of optical imaging probes. Nanomedicine (Lond).
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Feneley M.R., Jan H., Granowska M., Mather S.J., Ellison D., Glass J., Coptcoat M., Kirby R.S., Ogden C., Oliver R.T., Badenoch D.F., Chinegwundoh F.I., Nargund V.H., Paris A.M., Britton K.E. (2000). Imaging with prostate-specific membrane antigen (PSMA) in prostate cancer. Prostate Cancer Prostatic Dis.
7 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
8 Luthi-Carter R., Barczak A.K., Speno H., Coyle J.T. (1998). Molecular characterization of human brain N-acetylated alpha-linked acidic dipeptidase (NAALADase). J Pharmacol Exp Ther.
9 O'Keefe D.S., Uchida A., Bacich D.J., Watt F.B., Martorana A., Molloy P.L., Heston W.D. (2000). Prostate-specific suicide gene therapy using the prostate-specific membrane antigen promoter and enhancer. Prostate.
10 Ponsky L.E., Cherullo E.E., Starkey R., Nelson D., Neumann D., Zippe C.D. (2002). Evaluation of preoperative ProstaScint scans in the prediction of nodal disease. Prostate Cancer Prostatic Dis.
11 Jain R.K. (1999). Transport of molecules, particles, and cells in solid tumors. Annu Rev Biomed Eng.
12 Sundaresan G., Yazaki P.J., Shively J.E., Finn R.D., Larson S.M., Raubitschek A.A., Williams L.E., Chatziioannou A.F., Gambhir S.S., Wu A.M. (2003). 124I-labeled engineered anti-CEA minibodies and diabodies allow high-contrast, antigen-specific small-animal PET imaging of xenografts in athymic mice. J Nucl Med.
13 Chen Y., Dhara S., Banerjee S.R., Byun Y., Pullambhatla M., Mease R.C., Pomper M.G. (2009). A low molecular weight PSMA-based fluorescent imaging agent for cancer. Biochem Biophys Res Commun.
14 Chen Y., Pullambhatla M., Banerjee S.R., Byun Y., Stathis M., Rojas C., Slusher B.S., Mease R.C., Pomper M.G. (2012). Synthesis and biological evaluation of low molecular weight fluorescent imaging agents for the prostate-specific membrane antigen. Bioconjug Chem.